# 6-[^18^F]Fluoro-L-m-tyrosine

Chemical name: | 6-[^18^F]Fluoro-L-m-tyrosine
Abbreviated name: | 6-[^18^F]FMT
Synonym: | [^18^F]FMT
Agent Category: | Compound
Target: | Aromatic L−amino acid decarboxylase (AAAD)
Target Category: | Enzyme-substrate
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FMT%20OR%206-FMT%20OR%20%286-%5BAll%20Fields%5D%20fluoro%20m%20tyrosines%29)]

6-[^18^F]Fluoro-L-m-tyrosine (6-[^18^F]FMT) is a noncatecholic radioligand developed for positron emission tomography (PET) imaging of dopaminergic metabolism and function in the central nervous system (CNS). It is an analog of dihydroxyphenylalanine (L-DOPA) labeled with ^18^F, a positron emitter with a physical t_½_ of 109.7 min.

Dopamine is an important neurotransmitter that regulates and controls human movement, motivation, and cognition (1). It is also associated with human behaviors such as reward, reinforcement, and addiction. There are four main dopaminergic pathways in the CNS (2). Two pathways originating in the ventral tegmental area project toward the cortex and the limbic area, a third pathway projects from the hypothalamus projects toward the pituitary gland, and a fourth pathway projects from the substantia nigra to the striatum. Neurons located in these pathways release dopamine as a neurotransmitter at their terminals. There are five known dopamine receptor subtypes, D_1_-like or D_2_-like (3). The D_1_-like receptor subtypes (D_1_ and D_5_) coupled with the Gs protein activate adenylyl cyclase, and the D_2_-like subtypes (D_2_, D_3_, and D_4_) coupled with G proteins inhibit adenylate cyclase. Abnormal changes in the dopaminergic system can lead to pathological conditions such as Parkinson’s disease (PD), schizophrenia, Huntington’s disease, depression, Gilles de la Tourette syndrome, narcolepsy and other neuropsychiatric disorders (4).

Radiotracer imaging with specific radiolabeled molecular probes can measure pre-, post-, and intra-synaptic aspects of the dopaminergic system (4). [^18^F]Fluoro-L-dopa ([^18^F]FDOPA) was the first presynaptic probe developed by Firnau et al. (5) and the first molecular probe used by Garnett et al (6). to visualize human brain dopamine in vivo. Like endogenous L-DOPA, [^18^F]FDOPA is converted by aromatic L-amino acid decarboxylase (AAAD), an enzyme to the dopamine analog fluorodopamine. Thus, PET imaging of [^18^F]FDOPA allows in vivo visualization and assessment of dopamine function in the brain. However, the use of [^18^F]FDOPA is complicated by the peripheral metabolism of this agent. DeJesus et al. (7) proposed the synthesis and use of [^18^F]FMT and other tyrosine analogs as possible alternative dopamine probes because they lack the enediol moiety required of catecholamine-O-methyltransferase (COMT) substrates. Three isomers of [^18^F]FMT, 2-, 4-, and 6-[^18^F]FMT, were initially produced and studied (8). 6-[^18^F]FMT appeared most promising as early studies showed that it gave better image contrast and followed the dopaminergic pathway in a manner similar to that of [^18^F]FDOPA (9, 10). However, there is evidence that 6-[^18^F]FMT is distributed in monkey brain regions rich with AAAD-containing monoaminergic neurons which include dopaminergic, serotonergic, and noradrenergic neurons (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FMT%20OR%206-FMT%20OR%20%286-%5BAll%20Fields%5D%20fluoro%20m%20tyrosines%29%20AND%20synthesis)]

DeJesus et al. (7, 8) reported the synthesis of 6-[^18^F]FMT via direct electrophilic fluorination of D,L-m-tyrosine with acetyl[^18^F]hypofluorite ([^18^F]AcOF). [^18^F]F_2_ was produced from [^18^O]O_2_ by a two-bombardment method. The final labeled product was purified by high performance liquid chromatography (HPLC). HPLC analysis showed that approximately 80% of the D,L-m-tyrosine had reacted, and ^19^F-NMR analysis indicated that the final product was a mixture of 2-, 4-, and 6-[^18^F]FMT isomers in the proportion of approximately 36:11:52, respectively. The radiochemical yield was 71 ± 5% (n = 3; decay correction based on [^18^F]AcOF activity) after purification. The specific activity was 3.7-7.4 GBq/mmol (100-200 mCi)/mmol).

Namavari et al. (12) described the synthesis of 6-[^18^F]FMT based on a regioselective radiofluorodestannylation procedure. In this method, N-(trifluoroacetyl)-3-acetoxy-6-(trimethylstannyl)-L-phenylalanine ethyl ester was first synthesized as a precursor. The radiosynthesis was carried out by electrophilic fluorodestannylation of the precursor and followed by exhaustive deprotection of the acid, amine, and phenol. More than 99% of the 6-[^18^F]FMT was chemically and radiochemically pure. Chiral HPLC determined the enantiomeric purity to be >99% and the total tin determined by inductively coupled plasma spectrometry was <15 parts per billion (ppb). The total synthesis time was 60 min, and the radiochemical yield was 17% of the decay-corrected ^18^F activity recovered from the target.

VanBrocklin et al. (13) prepared a new di-Boc protected precursor, N-(tert-butoxycarbonyl)-3-(tert-butoxycarbonyloxy)-6-trimethylstannyl-L-phenylalanine ethyl ester for electrophilic fluorination. This precursor was synthesized from D,L-m-tyrosine in four steps with an overall yield of 26-27%. The enatiomeric purity was >95%. Decay-corrected radiochemical yields (n >6) for a two-pot method and one-pot method were 26 ± 3% and 25 ± 6%, respectively. For both methods, the chemical and radiochemical purities were >96%, and the range of specific activities of 6-[^18^F]FMT was 28-74 MBq/μmol (0.75-2 Ci/mmol). The amount of total tin was <5-40 ppb.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FMT%20OR%206-FMT%20OR%20%286-%5BAll%20Fields%5D%20fluoro%20m%20tyrosines%29%20AND%20in%20vitro%20studies)]

DeJesus et al. (14) used rat striatial synaptosomes to determine that the K_m_ and V_max_ of 6-[^18^F]FMT were 53 μM and 390 pmol/min/g, respectively. In contrast, L-DOPA had a K_m_ of 125 μM and V_max_ of 98 pmol/min per g. Nahmias et al. (15) found that in vitro incubation of 6-[^18^F]FMT in human whole blood showed that it took approximately 1 h for 6-[^18^F]FMT to equilibrate between plasma and erythrocytes. In comparison, [^18^F]fluorodeoxygluclose equilibrated instantaneously.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FMT%20OR%206-FMT%20OR%20%286-%5BAll%20Fields%5D%20fluoro%20m%20tyrosines%29%20AND%20rodentia)]

Barrio et al. (9) conducted regional brain distribution and peripheral metabolism of 6-[^18^F]FMT in rats. Each rat received 51.8 MBq/kg (1.4 mCi/kg) radioactivity by i.v. administration and 5 mg/kg carbidopa (AAAD inhibitor) subcutaneously 60 min before the radioligand injection. HPLC analysis of rat striatal tissue 30 min after injection revealed that the main metabolite (54 ± 4% of radioactivity) was 6-[^18^F]fluoro-m-tyramine (6-[^18^F]FMA), a product of AAAD-mediated decarboxylation. Without carbidopa pretreatment, both the cerebellum activity and total striatum activity of 6-[^18^F]FMA appeared to increase. Rahman et al. (16) reported that the AAAD activity in rat serum was 60 pmol/min per ml.

In an in vivo microdialysis study of striatal 6-[^18^F]FMT metabolism in conscious freely moving rats, Jordan et al. (17) injected benserazide (decarboxylation inhibitor, 50 mg/kg i.p.) 30-150 min before i.v. administration of 6-[^18^F]FMT (25 mg/kg). The study found that [^18^F]fluoro-3-hydroxyphenylacetic acid ([^18^F]FPAC ) was the major metabolite in the striatum at 20-120 min after injection. The concentrations of 6-[^18^F]FMT and [^18^F]FPAC were 0.2-0.3 nM (peak concentration within 20 min) and 3.2-3.3 nM (peak concentration within 40 min), respectively. [^18^F]FMA was below the limit of HPLC/electrochemical quantitation in all microdialysate samples. The authors suggested that 6-[^18^F]FMA existed briefly prior to its rapid oxidation into [^18^F]FPAC. The 6-[^18^F]FMT and [^18^F]FPAC concentration profiles were similar in control and reserpinized rats. Treatment with 2.5 mg/kg amphetamine i.p. at 120 min after 6-[^18^F]FMT injection caused a transient rise in the microdialysate [^18^F]FPAC concentration in control rats but not in reserpinized rats. The authors believed this was related to the ability of amphetamine to release presynaptic dopamine store. In addition, [^18^F]FMT and its metabolites peaked at 40 min and remained in the extracelluar space at a relatively constant level for the next 40-160 min after injection suggesting trapping of [^18^F]FPAC. In contrast, [^18^F]FDOPA and its metabolites, which also peaked at 40 min, cleared the brain with a t_½_ of about 2 h (18).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FMT%20OR%206-FMT%20OR%20%286-%5BAll%20Fields%5D%20fluoro%20m%20tyrosines%29%20AND%20%28primate%20NOT%20human%29)]

DeJesus et al. (10) conducted a comparison study between fluorinated m-tyrosine analogs and [^18^F]FDOPA in monkeys. Three monkeys were pretreated with carbidopa (2 mg/kg) 1 h before receiving 159.1-214.6 MBq (4.3-5.8 mCi) of 6-[^18^F]FMT. PET imaging up to 90 min showed that [^18^F]FDOPA had higher extracerebral radioactivity localization than 6-[^18^F]FMT. The striatum/cerebellum ratios at 85 min were 5.8 and 2.8 for 6-[^18^F]FMT and [^18^F]FDOPA, respectively. The mean K_i_ (min−^1^) values were 0.0187 ± 0.0005 (n =3) and 0.0089 ± 0.0005 (n = 5) for 6-[^18^F]FMT and [^18^F]FDOPA, respectively. HPLC analysis of blood metabolites showed that 6-[^18^F]FMT had two metabolites, and one was identified as 6-[^18^F]FPAC.

Jordan et al. (19) studied the kinetics and metabolism of 6-[^18^F]FMT in monkeys rendered hemi-Parkinsonian by unilateral intracarotid artery infusion of the neurotoxin 1-methyl-4-phenyl-1,2,3,6-tetrahydropyridine (MPTP). Four monkeys received 99.9 MBq/kg (2.7 mCi/kg) of 6-[^18^F]FMT (specific activity = 18.5 GBq/mM(0.5 Ci/mM) by i.v. administration. HPLC analysis of postmortem brain sections indicated that [^18^F]FPAC was the predominant metabolite with highest concentrations in dopaminergic regions at 60 and 120 min after injection. The 6-[^18^F]FMT metabolism profile was similar in treated and untreated animals. Other PET imaging studies used this MPTP monkey model to show that striatal 6-[^18^F]FMT uptake was altered in MPTP-treated animals (20-23). Both 6-[^18^F]FMT and [^18^F]FDOPA K_i_ values clearly differentiated MPTP-lesioned animals from normal animals (20). However, it was not possible to use 6-[^18^F]FMT k_loss_ (loss of radioactivity out of the striatum) or k_loss_/K_i_ (a measure of dopamine turnover) values to differentiate MPTP-lesioned animals from normal animals whereas it was possible with the [^18^F]FDOPA k_loss_ or k_loss_/K_i_ values. Another study comparing 6-[^18^F]FMT and [^18^F]FDOPA in aging monkeys suggested that 6-[^18^F]FMT might be more suitable for assessing CNS AAAD activity and that [^18^F]FDOPA might be better in tracing dopamine turnover (24). Eberling et al (25). proposed that 6-[^18^F]FMT PET imaging could be used to monitor AAAD gene expression by a simple ratio method.

In a study of 3 monkeys, Brown et al. (11) found that 6-[^18^F]FMT radioactivity localization did not correlate with dopamine concentration in other brain regions. On the other hand, localization of 6-[^18^F]FMT radioactivity appeared to significantly correlate with regional AAAD activity (r = 0.97). DeJesus et al. (24) used 6-[^18^F]FMT (118-222 MBq/dose (3.2-6 mCi/dose) PET imaging to study aging monkey brains. Insignificant correlation was found between 6-[^18^F]FMT radioactivity in young (3-11 years, n = 8) and older (25-37 years, n = 6) animals. The authors suggested that AAAD activity was maintained or increased in the aging monkey striatum. This result was confirmed by Eberling et al. (26). DeJesus et al (27). also reported that the in vivo turnover t_½_ of the enzyme AAAD in the striatum of normal monkeys after irreversible inhibition to be 86 h.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FMT%20OR%206-FMT%20OR%20%286-%5BAll%20Fields%5D%20fluoro%20m%20tyrosines%29%20AND%20human)]

Firnau et al. (28) studied the brain accumulation of 6-[^18^F]FMT and its synthesized metabolite, [^18^F]FPAC, up to 2 h in a healthy volunteer. The i.v. doses of both radiolabeled compounds were 111 MBq (3 mCi). The study reported that exogenously administered [^18^F]FPAC radioactivity in the brain was only about 5% of that of 6-[^18^F]FMT. In comparison, exogenous O-methylated (OMe[^18^F]DOPA) radioactivity accumulated to about ½ that of [^18^F]FDOPA radioactivity in all regions of the brain.

Nahmias et al. (29) performed 6-[^18^F]FMT PET imaging in 6 normal volunteers and 1 patient with PD. Each subject received 185-370 MBq (5-10 mCi; specific activity = 74 GBq/mM(2 Ci/mM) radioactivity and was not pretreated with carbidopa. In the normal volunteers, radioactivity accumulated in the dopamine-rich areas, the caudate nucleus and the putamen. In the PD patient, little radioactivity accumulation was observed in the putamen contralateral to the side exhibiting clinical symptoms. The mean striatum/cerebellum ratio was 4.95 ± 1.16 (n = 6), and the mean influx rate K_c_ for the striatum was 0.0171 ± 0.0018 ml/min per g. In comparison, [^18^F]FDOPA had a striatum/cerebellum ratio of 2.18 ± 0.22 (n = 19). Blood samples analyzed by chromatography indicated that the percentages of intact 6-[^18^F]FMT were 69% at 10 min and 49% at 90 min. In one volunteer who did a repeated study and was pretreated with 5 mg/kg carbidopa, the percentages of intact 6-[^18^F]FMT were 91% at 10 min and 70% at 90 min. The study also indicated that data from the striatal, cortical, and cerebellar time-activity curves were best fitted by a two-compartment, three-parameter model. Asselin et al. (30) in a study of blood data collected on 30 human subjects injected with 6-[^18^F]FMT proposed that a three-compartment four-parameter model gave significantly better fits to the blood data.

Asselin et al. (31) described striatal patterns of 6-[^18^F]FMT distribution in 21 patients for differential diagnoses of PD and other movement disorders. It was reported that the striatal 6-[^18^F]FMT distribution pattern can be used to classify patients by the following diagnoses: (a) normal, essential tremor and DOPA-responsive dystonia, (b) progressive supranuclear palsy and multiple system atrophy (MSA), (c) unilateral PD, (d) bilateral PD, MSA, and late-onset dystonia, and (e) corticobasal degeneration.

## References

1 Volkow ND, Fowler JS, Gatley SJ, Logan J, Wang GJ, Ding YS, Dewey S. (1996). PET evaluation of the dopamine system of the human brain. J Nucl Med.
2 Dailly E, Chenu F, Renard CE, Bourin M. (2004). Dopamine, depression and antidepressants. Fundam Clin Pharmacol.
3 3. Wagner HNJ, Szabo Z. Research and clinical applications of neuroreceptor imaging, in Handbook of Radiopharmaceuticals, M.J. Welch and C.S. Redvanly, Editors. 2003, John Wiley & Sons, Ltd: West Sussex, England. p. 582-602.
4 Verhoeff NP. (1999). Radiotracer imaging of dopaminergic transmission in neuropsychiatric disorders. Psychopharmacology (Berl).
5 Firnau G, Nahmias C, Garnett S. (1973). The preparation of (18 F)5-fluoro-DOPA with reactor-produced fluorine-18. Int J Appl Radiat Isot.
6 Garnett ES, Firnau G, Nahmias C. (1983). Dopamine visualized in the basal ganglia of living man. Nature.
7 DeJesus OT, Mukherjee J, Appelman EH. (1989). Synthesis of O- and M-thyrosine analogs as potential tracers for CNS dopamine. J. Label. Comp. Radiopharm.
8 DeJesus OT, Sunderland JJ, Nickles JR, Mukherjee J, Appelman EH. (1990). Synthesis of radiofluorinated analogs of m-tyrosine as potential L-dopa tracers via direct reaction with acetylhypofluorite. Int J Rad Appl Instrum [A].
9 Barrio JR, Huang SC, Yu DC, Melega WP, Quintana J, Cherry SR, Jacobson A, Namavari M, Satyamurthy N, Phelps ME. (1996). Radiofluorinated L-m-tyrosines: new in-vivo probes for central dopamine biochemistry. J Cereb Blood Flow Metab.
10 DeJesus OT, Endres CJ, Shelton SE, Nickles RJ, Holden JE. (1997). Evaluation of fluorinated m-tyrosine analogs as PET imaging agents of dopamine nerve terminals: comparison with 6-fluoroDOPA. J Nucl Med.
11 Brown WD, DeJesus OT, Pyzalski RW, Malischke L, Roberts AD, Shelton SE, Uno H, Houser WD, Nickles RJ, Holden JE. (1999). Localization of trapping of 6-[(18)F]fluoro-L-m-tyrosine, an aromatic L-amino acid decarboxylase tracer for PET. Synapse.
12 Namavari M, Satyamurthy N, Phelps ME, Barrio JR. (1993). Synthesis of 6-[18F] and 4-[18F]fluoro-L-m-tyrosines via regioselective radiofluorodestannylation. Appl Radiat Isot.
13 VanBrocklin HF, Blagoev M, Hoepping A, O'Neil JP, Klose M, Schubiger PA, Ametamey S. (2004). A new precursor for the preparation of 6-[18F]Fluoro-L-m-tyrosine ([18F]FMT): efficient synthesis and comparison of radiolabeling. Appl Radiat Isot.
14 DeJesus OT, Murali D, Nickles RJ. (1995). Synthesis of brominated and fluorinated ortho-tyrosine analogs as potential DOPA decarboxylase tracers. J Label. Comp. Radiopharm.
15 Nahmias C, Wahl LM, Amano S, Asselin MC, Chirakal R. (2000). Equilibration of 6-[18F]fluoro-L-m-tyrosine between plasma and erythrocytes. J Nucl Med.
16 Rahman MK, Nagatsu T, Kato T. (1981). Determination of aromatic L-amino acid decarboxylase in serum of various animals by high-performance liquid chromatography with electrochemical detection. Life Sci.
17 Jordan S, Bankiewicz KS, Eberling JL, VanBrocklin HF, O'Neil JP, Jagust WJ. (1998). An in vivo microdialysis study of striatal 6-[18F]fluoro-L-m-tyrosine metabolism. Neurochem Res.
18 DeJesus OT, Haaparanta M, Solin O, Nickles RJ. (2000). 6-fluoroDOPA metabolism in rat striatum: time course of extracellular metabolites. Brain Res.
19 Jordan S, Eberling JL, Bankiewicz KS, Rosenberg D, Coxson PG, VanBrocklin HF, O'Neil JP, Emborg ME, Jagust WJ. (1997). 6-[18F]fluoro-L-m-tyrosine: metabolism, positron emission tomography kinetics, and 1-methyl-4-phenyl-1,2,3,6-tetrahydropyridine lesions in primates. Brain Res.
20 Doudet DJ, Chan GL, Jivan S, DeJesus OT, McGeer EG, English C, Ruth TJ, Holden JE. (1999). Evaluation of dopaminergic presynaptic integrity: 6-[18F]fluoro-L-dopa versus 6-[18F]fluoro-L-m-tyrosine. J Cereb Blood Flow Metab.
21 Eberling JL, Jagust WJ, Taylor S, Bringas J, Pivirotto P, VanBrocklin HF, Bankiewicz KS. (1998). A novel MPTP primate model of Parkinson's disease: neurochemical and clinical changes. Brain Res.
22 Eberling JL, Pivirotto P, Bringas J, Bankiewicz KS. (2000). Tremor is associated with PET measures of nigrostriatal dopamine function in MPTP-lesioned monkeys. Exp Neurol.
23 Eberling JL, Pivirotto P, Bringas J, Bankiewicz KS. (2004). Comparison of two methods for the analysis of [18F]6-fluoro-L-m-tyrosine PET data. Neuroimage.
24 Dejesus OT, Endres CJ, Shelton SE, Nickles RJ, Holden JE. (2001). Noninvasive assessment of aromatic L-amino acid decarboxylase activity in aging rhesus monkey brain in vivo. Synapse.
25 Eberling JL, Cunningham J, Pivirotto P, Bringas J, Daadi MM, Bankiewicz KS. (2003). In vivo PET imaging of gene expression in Parkinsonian monkeys. Mol Ther.
26 Eberling JL, Roberts JA, Taylor SE, VanBrocklin HF, O'Neil JP, Nordahl TE. (2002). No effect of age and estrogen on aromatic L- amino acid decarboxylase activity in rhesus monkey brain. Neurobiol Aging.
27 DeJesus OT, Flores LG, Murali D, Converse AK, Bartlett RM, Barnhart TE, Oakes TR, Nickles RJ. (2005). Aromatic L-amino acid decarboxylase turnover in vivo in rhesus macaque striatum: a microPET study. Brain Res.
28 Firnau G, Chirakal R, Nahmias C, Garnett ES. (1991). Do the metabolites of [18F]Fluoro-L-Dopa and [18F]Fluoro-meta-Tyrosine contribute to the accumulation of [18F] in the human brain?. Label. Comp. Radiopharm.
29 Nahmias C, Wahl L, Chirakal R, Firnau G, Garnett ES. (1995). A probe for intracerebral aromatic amino-acid decarboxylase activity: distribution and kinetics of [18F]6-fluoro-L-m-tyrosine in the human brain. Mov Disord.
30 Asselin MC, Wahl LM, Cunningham VJ, Amano S, Nahmias C. (2002). In vivo metabolism and partitioning of 6-[18F]fluoro-L-meta-tyrosine in whole blood: a unified compartment model. Phys Med Biol.
31 31. Asselin MC, Amano S, Chirakal R, Thompson M, Nahmias C. Patterns of distribution of [18F]6fluoro-L-m-tyrosine in PET images of pateints with movement disorders, in Brain Imaging Using PET, M. Senda, Y. Kimura, and P. Herscovitch, Editors. 2002, New York Academic Press: New York.